# 6,7-Dimethoxy-2-[3-(5-[^11^C]methoxy-1,2,3,4-tetrahydro-naphthalen-1-yl)-propyl]-1,2,3,4-tetrahydro-isoquinoline

Chemical name: | 6,7-Dimethoxy-2-[3-(5-[^11^C]methoxy-1,2,3,4-tetrahydro-naphthalen-1-yl)-propyl]-1,2,3,4-tetrahydro-isoquinoline
Abbreviated name: | [^11^C]MC-266, [11C]7
Synonym:
Agent category: | Compound
Target: | P-glycoprotein multidrug transporter, MDR-1
Target category: | Transporter
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20P-gp)]

One of the mechanisms of tumor cells to escape the cytotoxic effects of chemotherapeutic agents, such as adriamycin, vinca alkaloids, epipodophyllotoxins, actinomycin D, and paclitaxel, is to limit their presence inside the cells by way of a multidrug resistance (MDR-1) gene protein (1, 2). The MDR-1 gene encodes a transmembrane P-glycoprotein (P-gp) as an ATP-dependent multidrug transporter that is capable of actively pumping a variety of agents out of the cells. Injection of unlabeled efflux pump substrates increases the retention of the radioactivity in the tumor by blocking the efflux rather than reducing radioactivity as seen with receptor-binding radiotracer blocking studies. Overexpression of P-gp in tumor cells (such as renal carcinoma, hepatoma, pheochromocytoma, and colon carcinoma) leads to resistance to anticancer drugs (3). P-gp is also present in a variety of normal cells, such as intestinal mucosal cells, hepatocytes, renal proximal tubule epithelial cells, and endothelial cells of the blood–brain barrier (BBB) (4, 5). Calcium channel blockers (such as verapamil), cyclosporine (CsA, P-gp inhibitor) and CsA's non-immunosuppressive analog PSC 833 (other mechanism) are MDR modulators that inhibit the transport of P-gp substrates out of the cells (6, 7).

^99m^Tc-Sestamibi (MIBI) has been approved by the United States Food and Drug Administration as a myocardial perfusion imaging agent for use with single-photon emission computed tomography to assess the risk of future cardiac events (8). It is also used as a tumor-imaging agent in breast, lung, thyroid, and brain cancers (8-10). MIBI is a substrate for P-gp (4, 11). 6,7-Dimethoxy-2-[3-(5-methoxy-1,2,3,4-tetrahydro-naphthalen-1-yl)-propyl]-1,2,3,4-tetrahydro-isoquinoline (MC-266) is another substrate for P-gp (12). [^11^C]MC-266 has been developed as a positron emission tomography (PET) agent for the non-invasive study of the P-gp function and MDR in tumors and normal tissues (13).

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=P-glycoprotein%5BAll+Fields%5D+AND+micad%5Bbook%5D) (P-glycoprotein)
- Gene information in NCBI (P-glycoprotein (http://www.ncbi.nlm.nih.gov/gene/5243))
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=omim&Cmd=DetailsSearch&Term=P-glycoprotein%5BAll+Fields%5D) (P-glycoprotein)
- Clinical trials (P-glycoprotein (http://www.clinicaltrials.gov/ct2/results?term=P-glycoprotein))
- Drug information in FDA (^99m^Tc-MIBI (http://google2.fda.gov/search?q=99mTc-sestamibi+&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=16))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20P-gp%20and%20synthesis)]

[^11^C]MC-266 was synthesized by reaction of the desmethyl precursor with [^11^C]methyl iodide for 4 min at 80°C (13). The radiochemical purity of purified [^11^C]MC-266 was >98% with a specific activity of >100 GBq/µmol (2.7 Ci/µmol) at the end of synthesis. The total synthesis time was 45 min with a radiochemical yield of ~30%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20P-gp%20and%20in%20vitro)]

Colabufo et al. (12) showed that MC-266 (5 µM) increased the intracellular uptake of doxorubicin in MCF7/adr cells by 4.8-fold and potentiated the anti-proliferation effect of doxorubicin (5 µM) from 5% to 85%. MC-266 activated ATPase of Caco-2 the monolayer. Therefore, MC-266 was classified as a P-gp substrate.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20P-gp%20and%20rodentia)]

van Waarde et al. (13) performed ex vivo biodistribution studies with 30–40 MBq (0.8–1.1 mCi) [^11^C]MC-266 in control rats (n = 5) and CsA-treated (50 mg/kg) rats (n = 4) at 60 min after injection. CsA is a P-gp inhibitor. The accumulation of radioactivity expressed as standard uptake value (SUV) in various brain regions was 0.30–0.50. Pretreatment with CsA increased the accumulation into the various brain regions by 1.0- to 2.5-fold (P < 0.05). The peripheral organ with the highest SUV was the liver (3.27), followed by the pancreas (3.16), spleen (1.64), and kidney (1.45). CsA did not affect the accumulation of radioactivity in any peripheral organ.

PET imaging showed an initial high accumulation in the brains of both control and CsA-treated rats at 0.5 min after injection, followed by an exponential washout. CsA exhibited a 1.5-fold increase in brain radioactivity at 25 min after [^11^C]MC-266 injection. The brain SUV was 0.88 for the control rats and 2.17 for the CsA-treated rats. Logan plot analysis with arterial input showed that CsA treatment increased the cerebral distribution volume from 1.86 to 5.26 (P < 0.002) and the influx rate constant from 0.18 to 0.64 (P < 0.0001). As a comparison at 25 min after injection, [^11^C]verapamil exhibited a lower SUV (0.15), which increased to 1.34 with CsA treatment. Logan plot analysis with arterial input showed that CsA treatment increased the cerebral distribution volume from 0.64 to 5.85 (P < 0.0001) and the influx rate constant from 0.22 to 0.81 (P < 0.002).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20P-gp%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20P-gp%20and%20%28nonhuman%20primate%29)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20P-gp%20and%20%28%20human%29)]

No publications are currently available.

## References

1 Endicott J.A., Ling V. (1989). The biochemistry of P-glycoprotein-mediated multidrug resistance. Annu Rev Biochem.
2 Gottesman M.M., Pastan I. (1993). Biochemistry of multidrug resistance mediated by the multidrug transporter. Annu Rev Biochem.
3 Fojo A.T., Ueda K., Slamon D.J., Poplack D.G., Gottesman M.M., Pastan I. (1987). Expression of a multidrug-resistance gene in human tumors and tissues. Proc Natl Acad Sci U S A.
4 Piwnica-Worms D., Rao V.V., Kronauge J.F., Croop J.M. (1995). Characterization of multidrug resistance P-glycoprotein transport function with an organotechnetium cation. Biochemistry.
5 Thiebaut F., Tsuruo T., Hamada H., Gottesman M.M., Pastan I., Willingham M.C. (1987). Cellular localization of the multidrug-resistance gene product P-glycoprotein in normal human tissues. Proc Natl Acad Sci U S A.
6 Hughes C.S., Vaden S.L., Manaugh C.A., Price G.S., Hudson L.C. (1998). Modulation of doxorubicin concentration by cyclosporin A in brain and testicular barrier tissues expressing P-glycoprotein in rats. J Neurooncol.
7 Mayer U., Wagenaar E., Dorobek B., Beijnen J.H., Borst P., Schinkel A.H. (1997). Full blockade of intestinal P-glycoprotein and extensive inhibition of blood-brain barrier P-glycoprotein by oral treatment of mice with PSC833. J Clin Invest.
8 Olszowska M., Kostkiewicz M., Tracz W., Przewlocki T. (2003). Assessment of myocardial perfusion in patients with coronary artery disease. Comparison of myocardial contrast echocardiography and 99mTc MIBI single photon emission computed tomography. Int J Cardiol.
9 Benard F., Romsa J., Hustinx R. (2003). Imaging gliomas with positron emission tomography and single-photon emission computed tomography. Semin Nucl Med.
10 Peng N.J., Chang H.T., Tsay D.G., Liu R.S. (2003). Technetium-99m-sestamibi scintimammography to detect breast cancer in patients with paraffinomas or siliconomas after breast augmentation. Cancer Biother Radiopharm.
11 Piwnica-Worms D., Kronauge J.F., Holman B.L., Lister-James J., Davison A., Jones A.G. (1988). Hexakis(carbomethoxyisopropylisonitrile) technetium(I), a new myocardial perfusion imaging agent: binding characteristics in cultured chick heart cells. J Nucl Med.
12 Colabufo N.A., Berardi F., Cantore M., Perrone M.G., Contino M., Inglese C., Niso M., Perrone R., Azzariti A., Simone G.M., Porcelli L., Paradiso A. (2008). Small P-gp modulating molecules: SAR studies on tetrahydroisoquinoline derivatives. Bioorg Med Chem.
13 van Waarde A., Ramakrishnan N.K., Rybczynska A.A., Elsinga P.H., Berardi F., de Jong J.R., Kwizera C., Perrone R., Cantore M., Sijbesma J.W., Dierckx R.A., Colabufo N.A. (2009). Synthesis and preclinical evaluation of novel PET probes for P-glycoprotein function and expression. J Med Chem.